# ^64^Cu-4,11-Bis(carboxymethyl)-1,4,8,11-tetraazabicyclo[6.6.2]hexadecane-D-Phe-cyclo(Cys-Tyr-D-Trp-Lys-Thr-Cys)-Thr(OH)

Chemical name: | ^64^Cu-4,11-Bis(carboxymethyl)-1,4,8,11-tetraazabicyclo[6.6.2]hexadecane-D-Phe-cyclo(Cys-Tyr-D-Trp-Lys-Thr-Cys)-Thr(OH)
Abbreviated name: | ^64^Cu-CB-TE2A-Y3-TATE
Synonym:
Agent category: | Peptide
Target: | Somatostatin receptor (sst_2_)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=47117741), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=71979669) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=6750) for more information about somatostatin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Y3-TATE)]

Somatostatin (SST) is an inhibitor of the release of somatotropin, glucagon, insulin, gastrointestinal hormones, and other secretory proteins (1). SST is also known as somatotropin release-inhibiting factor (SRIF). SST is a cyclic polypeptide with two biologically active isoforms, SRIF-14 and SRIF-28, of 14 and 28 amino acids, respectively. SRIF has a short plasma half-life of <3 min (2). SST receptors (SSTRs) (G-protein–coupled) have been found on a variety of neuroendocrine tumors and cells of the immune system, and five individual subtypes (sst_1_–sst_5_) have been identified and subsequently cloned from animal and human tissues (3, 4). SST also inhibits cell proliferation and promotes apoptosis through binding to specific cell-surface SSTRs (5).

^111^In-Labeled diethylenetriaminepentaacetic acid-octreotide (^111^In-DTPA-OCT) is an SSTR analog that, over the last decade, has remained the most widely used radiopharmaceutical for the scintigraphic detection and staging of primary and metastatic neuroendocrine tumors bearing SSTRs with single-photon emission computed tomography (SPECT) (6). It has also shown promising results in peptide-receptor radionuclide therapy (7). OCT is a cyclic peptide with eight amino acids (D-Phe-cyclo(Cys-Phe-D-Trp-Lys-Thr-Cys)-Thr(OH)). ^111^In-DTPA-OCT binds with high affinity to SSTR subtypes 2 and 5 (sst_2_ and sst_5_) and to sst_3_ to a lesser degree, but it does not bind to sst_1_ or sst_4_ (8). Currently used targeting SSTR peptides mainly have affinity for sst_2_. D-Phe-cyclo(Cys-Tyr-D-Trp-Lys-Thr-Cys)-Thr(OH) ([Tyr3]-octreotate (Y3-TATE)) was found to be a selective sst_2_ agonist. For evaluation as a positron emission tomography (PET) imaging agent for sst_2_, ^64^Cu has been attached to Y3-TATE via bis(carboxymethyl)-1,4,8,11-tetraazabicyclo[6.6.2]hexadecane (CB-TE2A) to form ^64^Cu-CB-TE2A-Y3-TATE (9).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Y3-TATE+and+synthesis)]

CB-TE2A-Y3-TATE was synthesized with standard solid-phase peptide synthesis with a calculated mass of 1,373.6 Da in agreement with mass spectrometry (9). CB-TE2A-Y3-TATE was purified with high-performance liquid chromatography. ^64^Cu was complexed to CB-TE2A-Y3-TATE by reaction of 0.7–10.7 nmol CB-TE2A-Y3-TATE with 37–555 MBq (1–15 mCi) ^64^CuCl_2_ in 0.1 M ammonium acetate (pH 8.0) for 1 h at 95°C. ^64^Cu-CB-TE2A-Y3-TATE had a >95% radiochemical purity and a specific activity of 188 GBq/µmol (5.1 Ci/µmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Y3-TATE+and+in+vitro)]

Sprague et al. (9) determined that ^64^Cu-CB-TE2A-Y3-TATE showed a K_d_ (affinity constant) of 1.7 nM and a B_max_ (receptor density) of 1.6 pmol/mg protein in AR42J (sst_2_-positive) tumor cell homogenates. On the other hand, ^64^Cu-TETA-Y3-TATE (sst_2_-selective agonist) exhibited a K_d_ of 0.7 nM and a B_max_ of 0.19 pmol/mg protein. Reubi et al. (10) reported that DTPA-Y3-TATE had 50% inhibition concentration (IC_50_) values of >1,000, 3.9 ± 1.0, >1,000, >1,000, and >1,000 nM for human sst_1_, sst_2_, sst_3_, sst_4_, and sst_5_ receptors in competition with ^125^I-SRIF-28, respectively. Both ^64^Cu-CB-TE2A-Y3-TATE and ^64^Cu-TETA-Y3-TATE were internalized into AR42J cells in culture, and the internalization was blocked by excess Y3-TATE. ^64^Cu-CB-TE2A-Y3-TATE internalization was higher than ^64^Cu-TETA-Y3-TATE at 15–60 min with no difference at 120 and 240 min.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Y3-TATE+and+rodentia)]

Sprague et al. (9) performed ex vivo biodistribution studies with ^64^Cu-CB-TE2A-Y3-TATE in rats (n = 4/group) bearing xenografts of AR42J tumor cells. The accumulation of radioactivity in the sst_2_ tumors was 6.0% injected dose per gram (% ID/g) at 1 h, 5.8% ID/g at 4 h, and 1.7% ID/g at 24 h after injection. The adrenal was the organ that had the highest accumulation at 4 h after injection (15% ID/g), followed by the pancreas (12% ID/g), kidney (4% ID/g), and liver (0.2% ID/g). The concentration in the blood and muscle was <0.1% ID/g with a tumor/blood ratio of 155 and a tumor/muscle ratio of 243 at 4 h after injection. Co-injection with Y3-TATE reduced the accumulation of radioactivity by 66% in the tumors, >90% in the adrenal, and >90% in the pancreas at 4 h after injection. Little or no inhibition was observed in the other tissues. The bone was not studied, but Wadas et al. (11) showed that co-injection with Y3-TATE inhibited the accumulation in the bone by 90%. The accumulation values for ^64^Cu-TETA-Y3-TATE in the tumor, adrenal, and pancreas were significantly lower (P < 0.005) than accumulation for ^64^Cu-CB-TE2A-Y3-TATE at 1, 4, and 24 h after injection. Whole-body SPECT imaging visualized the sst_2_ tumor as early as 1 h after injection of ^64^Cu-CB-TE2A-Y3-TATE. The tumor standard uptake values (SUVs) were 2.0, 1.5, and 0.8 at 1, 4, and 24 h, respectively. The kidney SUVs were 2.5, 2.2, and 1.8 at 1, 4, and 24 h, respectively. The liver SUVs were >0.5 at these time points. The tumor SUVs for ^64^Cu-TETA-Y3-TATE were 1.5 at 1 h and 1.0 at 4 h after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Y3-TATE+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Y3-TATE+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Y3-TATE+and+human)]

No publication is currently available.

## NIH Support

R01 CA064475, R01 EB004533, R24 CA86307

## References

1 Weckbecker G., Lewis I., Albert R., Schmid H.A., Hoyer D., Bruns C. (2003). Opportunities in somatostatin research: biological, chemical and therapeutic aspects. Nat Rev Drug Discov.
2 Patel Y.C., Wheatley T. (1983). In vivo and in vitro plasma disappearance and metabolism of somatostatin-28 and somatostatin-14 in the rat. Endocrinology.
3 Corleto V.D., Nasoni S., Panzuto F., Cassetta S., Delle Fave G. (2004). Somatostatin receptor subtypes: basic pharmacology and tissue distribution. Dig Liver Dis.
4 Moller L.N., Stidsen C.E., Hartmann B., Holst J.J. (2003). Somatostatin receptors. Biochim Biophys Acta.
5 Barnett P. (2003). Somatostatin and somatostatin receptor physiology. Endocrine.
6 Krenning E.P., Kwekkeboom D.J., Bakker W.H., Breeman W.A., Kooij P.P., Oei H.Y., van Hagen M., Postema P.T., de Jong M., Reubi J.C., et al. (1993). Somatostatin receptor scintigraphy with [111In-DTPA-D-Phe1]- and [123I-Tyr3]-octreotide: the Rotterdam experience with more than 1000 patients. Eur J Nucl Med.
7 Kwekkeboom D.J., Mueller-Brand J., Paganelli G., Anthony L.B., Pauwels S., Kvols L.K. (2005). M. O'Dorisio T, R. Valkema, L. Bodei, M. Chinol, H.R. Maecke, and E.P. Krenning, Overview of results of peptide receptor radionuclide therapy with 3 radiolabeled somatostatin analogs. J Nucl Med.
8 Storch D., Behe M., Walter M.A., Chen J., Powell P., Mikolajczak R., Macke H.R. (2005). Evaluation of [99mTc/EDDA/HYNIC0]octreotide derivatives compared with [111In-DOTA0,Tyr3, Thr8]octreotide and [111In-DTPA0]octreotide: does tumor or pancreas uptake correlate with the rate of internalization?. J Nucl Med.
9 Sprague J.E., Peng Y., Sun X., Weisman G.R., Wong E.H., Achilefu S., Anderson C.J. (2004). Preparation and biological evaluation of copper-64-labeled tyr3-octreotate using a cross-bridged macrocyclic chelator. Clin Cancer Res.
10 Reubi J.C., Schar J.C., Waser B., Wenger S., Heppeler A., Schmitt J.S., Macke H.R. (2000). Affinity profiles for human somatostatin receptor subtypes SST1-SST5 of somatostatin radiotracers selected for scintigraphic and radiotherapeutic use. Eur J Nucl Med.
11 Wadas T.J., Eiblmaier M., Zheleznyak A., Sherman C.D., Ferdani R., Liang K., Achilefu S., Anderson C.J. (2008). Preparation and biological evaluation of 64Cu-CB-TE2A-sst2-ANT, a somatostatin antagonist for PET imaging of somatostatin receptor-positive tumors. J Nucl Med.